# ^99m^Tc/^111^In-Labeled DTPA-succinyl polylysine

Chemical name: | ^99m^Tc/^111^In-Labeled DTPA-succinyl polylysine
Abbreviated name: | [^99m^Tc/^111^In]-DSPL
Synonym:
Agent Category: | Ligand
Target: | Bombesin anti-DTPA bispecific antibody complexes
Target Category: | Antibody
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc/^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bispecific%20antibodies&cmd=DetailsSearch)]

Intact radiolabeled monoclonal antibodies (mAbs) or their derivatives that are used for the immunotherapy of cancer have limited efficacy because they have low tumor penetration due to their large size (~150 kDa); in addition, radiolabeled Abs are not very useful to visualize cancerous lesions with different imaging modalities (primarily positron emission tomography (PET) and single-photon emission computed tomography (SPECT)) due to their long circulation half-life values (1). In addition, radioactivity derived from the directly labeled mAbs (or their derivatives) tends to accumulate in organs such as the liver, where the proteins are catabolized, and the tumors can be visualized only after a prolonged exposure to the tracer. To amplify the signal obtained from an imaging agent that can be used for the noninvasive detection of malignant tumors, a strategy of pretargeting the neoplastic lesions with a bispecific monoclonal antibody (bsmAb) was developed and evaluated in preclinical studies as discussed in detail by Sharkey et al. (2). To summarize this strategy, neoplastic lesions in the animals are first pretargeted with a suitable bsmAb (or its derivative) that binds to a tumor antigen with one arm. The animals are then injected with an appropriate radionuclide-chelator complex that binds to the second arm of the bsmAb complex. Because the radiolabeled chelator complex is a small molecular weight ligand, the excess tracer complex is cleared rapidly from circulation and non-target tissues by the kidneys. Therefore, the pretargeting technique generates higher signal/noise ratios compared to those obtained with the directly labeled mAb alone, and the lesions can be visualized with either PET or SPECT (2).

A preclinical study was performed to evaluate the use of a radiolabeled ligand with SPECT to detect minute cancerous xenograft tumors in rodents that had been pretargeted with a bsmAb. This study showed that the lesions were not easily visualized because the radiochemical had a low specific target binding (3). In another study, experimental atherosclerotic plaques in mice were pretargeted with a bsmAb, and a high-specific activity, ^99m^Tc-labeled, negatively charged polymer (^99m^Tc-labeled DTPA-succinyl-polylysine ([^99m^Tc]-DSPL)) was used to target the bsmAb to visualize the lesions with gamma planar imaging (3). With this approach, the lesions were reported to have a very high signal/noise ratio and were visible as soon as 2 h postinjection (p.i.). A similar procedure was used with [^99m^Tc]-DSPL to visualize metastatic melanoma lung lesions in mice (4). Patil et al. successfully used ^99m^Tc/^111^In-labeled-DSPL ([^99m^Tc/^111^In]-DSPL) with SPECT to detect pretargeted PC-3 cell human prostate cancer xenograft tumors in severe combined immunodeficient mice (SCID) (5).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Bispecific%20antibodies%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DTPA-succinylated-polylysine&cmd=DetailsSearch)]

The synthesis and the labeling of DSPL with ^99m^Tc has been described by Gada et al. (4). The specific activity (SA) of [^99m^Tc]-DSPL was 192–505 MBq/nmol (7.1 mCi–18.68 mCi/nmol). The radiochemical yield (RCY), radiochemical purity (RCP), and stability of the ^99m^Tc-labeled polymer were not reported.

[^111^In]-DSPL was synthesized for use in some studies (5). The SA, RCY, RCP, and stability of this labeled polymer were also not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D-DTPA-succinylated-polylysine%20in%20vitro&cmd=DetailsSearch)]

No reference is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D-DTPA-succinylated-polylysine%20rodentia&cmd=DetailsSearch)]

The use of [^99m^Tc]-DSPL was evaluated for the visualization of atherosclerotic lesions caused by proliferating smooth muscle cells in the femoral arteries of ApoE knockout mice and pretargeted with a Z2D3-F(ab')_2_-anti-DTPA-F(ab')_2_ bsmAb (Z2D3 is a murine chimeric Ab that specifically binds to an as yet uncharacterized complex lipid antigen that is produced only by proliferating smooth muscle cells) (3). For this study, Sprague-Dawley rats (n = 5 animals) were given an intramuscular injection of surrogate Z2D3 antigen-coated polystyrene beads (SAB) in the right hind leg; for use as controls, an equal number of unmodified beads (UMB) were injected into the left hind leg of the animals (3). The following day, all the animals were given an intravenous injection of the bsmAb, and 24 h later each animal was injected with 6.6 MBq (0.18 mCi) [^99m^Tc]-DSPL. Serial gamma planar whole-body images of the animals were recorded at 2 h and 24 h after the [^99m^Tc]-DSPL injection. At 2 h p.i., the SAB lesions were visible, but radioactivity was observed in the blood pool as well. At 24 h p.i., the SAB lesions, the liver, kidneys, and the bladder of the animals were clearly visible in the posteroanterior images of the rodents. Following the imaging session, the animals were euthanized, and normal thoracic muscle tissue and muscle areas injected with the SAB and the UMB were excised to determine the amount radioactivity present in the tissues. All results were presented as % of injected dose per gram tissue (% ID/g). Right leg muscle tissue harvested from four of the five rats injected with the bsmAb-coated polymer showed a significantly higher accumulation (P = 0.03) of radioactivity (0.000822 ± 0.00019% ID/g) compared with either the UMB (0.000525 ± 0.00017% ID/g) or the thoracic muscle (0.000467 ± 0.00017% ID/g; P = 0.01) areas. Presence of SAB in the right leg muscle area was confirmed by microscopic examination of the tissue.

In another study with rats (n = 4 animals), it was shown that femoral deendothelialization lesions in the left leg of the animals that were pretargeted with Z2D3-F(ab')_2_-anti-DTPA-F(ab')_2_ bsmAb could be visualized with [^99m^Tc]-DSPL (3). The mean ratio of tracer in the left femoral artery segment was 1.8 ± 0.7-fold higher (P = 0.04) than the control femoral artery segment in the right leg of the same animals.

Lung metastatic melanoma lesions pretargeted with the 2C5–6C31H3 bsMAb (prepared by conjugating an antinucleosomal targeting Ab (2C5) that recognizes a nucleosomal pan cancer antigen with an anti-DTPA Ab (6C31H3; the capturing Ab)) could be visualized using [^99m^Tc]-DSPL with SPECT (4). Mice (n = 5 animals) bearing B16-F10 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-6475&Template=cellBiology) metastatic tumors in the lungs were injected intravenously (i.v.) with 10 μg 2C5–6C31H3 bsmAb to pretarget the lesions 24 h before the imaging session (4). Control animals (n = 4 mice) bearing the tumors did not receive the pretargeting bsmAb. All the animals received an i.v. injection of ~37 MBq (~1.34 mCi) [^99m^Tc]-DSPL, and gamma planar images of the rodents were acquired at various time points ranging from 1 h p.i. to 24 h p.i. At 1 h p.i., the metastatic lesions were visible in the lungs of the pretargeted animals, but not in the non-pretargeted mice. In all the animals, the label was rapidly cleared through the kidneys, and there was little accumulation of the tracer in the liver. Presence of radioactivity in the lung lesions was confirmed with SPECT/computed tomography imaging.

The biodistribution of [^99m^Tc]-DSPL was studied in mice bearing lung metastatic melanoma lesions pretargeted with the 2C5–6C31H3 bsmAb (n = 5 animals) (4). For use as controls, non-pretargeted mice bearing lung metastatic melanoma lesions were injected with [^99m^Tc]-DSPL alone (n = 4 animals). Another group of normal mice (without the metastatic lesions in the lungs) were pretargeted with bsMab or the anti-DTPA Ab and injected with [^99m^Tc]-DSPL (n = 3 animals/treatment group). To determine the amount of radioactivity accumulated in the various organs of interest, all the animals were euthanized at 24 h p.i. The amount of label accumulated in the whole lungs of the pretargeted group was 3.20 ± 2.06% ID/g, which was significantly higher than the uptake of radioactivity in the lungs of the control group (0.40 ± 0.15% ID/g; P = 0.01). The amount of radioactivity in the lungs of normal animals injected with the bsMab or the anti-DTPA Ab was 0.15 ± 0.01% ID/g (P ≤ 0.001 and P = 0.032 for the bsMab or the anti-DTPA Ab mice, respectively). The lung to liver ratio of the bsMAb-pretreated animals was reported to be 5.25.

[^99m^Tc/^111^In]-DSPL was shown to be suitable for the visualization of bsmAb-pretargeted human prostate cancer PC-3 cell xenograft tumors in SCID mice (5). For these studies, the intact 6C31H3 anti-DTPA Ab and its Fab' fragment were linked to the bombesin peptide to obtain Bom-bsCx and Bom-bsFx, respectively. Bombesin has a very high affinity for the gastrin-releasing peptide receptors (Bom; also designated as the Bom receptor) that are overexpressed on PC-3 cells. In separate studies, mice bearing the PC-3 cell tumors were pretargeted with Bom-bsCx and Bom-bsFx, respectively, and [^99m^Tc/^111^In]-DSPL was used to visualize the lesions with scintigraphy (5). At the end of the imaging session, the rodents were euthanized, and all organs of interest were retrieved to determine the amount of radioactivity accumulated in the different tissues.

In the first study, mice bearing the xenograft tumors were pretargeted with an injection of Bom-bsCx (n = 4 animals) (5). Control animals were pretargeted with either 6C31H3 alone (n = 3 animals) or Bom alone (n = 2 animals). Twenty-four hours later, the animals (under anesthesia) were injected with 7.03 ± 1.74 MBq (259 ± 64.38 μCi) or 6.88 ± 1.89 MBq (373 ± 69.93 μCi) [^111^In]-DSPL for gamma planar imaging at time points ranging from 5 min p.i. to 24 h p.i. From the images it was evident that the radioactivity was excreted rapidly through the kidneys, and there was little accumulation of tracer in the liver or heart of the animals. The xenograft tumors were clearly visible within 1–3 h p.i. in animals pretargeted with Bom-bsCx. No lesions were visible in the control animals. The amount of radioactivity accumulated in tumors of animals pretargeted with Bom-bcCx was 1.21 ± 0.35% ID/g, which was ~5.5-fold higher than accumulation in tumors in mice pretreated with either Bom or 6C31H3 alone (0.22 ± 0.08% ID/g; P = 0.001). The amount of radioactivity detected in the liver, spleen, and salivary glands of animals pretargeted with Bom-bcCx were ~0.5% ID/g, ~0.4% ID/g, and ~0.4% ID/g, respectively.

In the second study, the mice bearing PC-3 cell xenograft tumors were pretargeted with Bom-bsFx (n = 4 animals), and the control animals (n = 3 mice) were pretargeted with Bom alone. For scintigraphy the animals were injected with 50.0 ± 5.34 MBq (1.85 ± 0.18 mCi) [^99m^Tc]-DSPL 24 h later, and whole-body images were acquired from the rodents as described above. No accumulation of radioactivity was observed in the liver of these animals, and the tracer was excreted primarily through the kidneys. With [^99m^Tc]-DSPL, the lesions were visible in the animals within 1–3 h p.i. At 24 h p.i., the uptake of radioactivity from [^99m^Tc]-DSPL in the tumors was 15-fold higher than that in the control lesions (6.54 ± 1.58% ID/g versus 0.44 ± 0.17% ID/g; P = 0.002). The amount of tracer in the liver and spleen of animals pretargeted with Bom-bsFx was ~2.0% ID/g and ~1.5% ID/g, respectively. All other organs showed an accumulation of <1.0% ID/g radioactivity.

From these studies, the investigators concluded that [^99m^Tc/^111^In]-DSPL can be used for the detection of minute tumors that have been pretargeted with an appropriate bsMab (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D-DTPA-succinylated-polylysine%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D-DTPA-succinylated-polylysine%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28Human%5BAll%20Fields%5D%20AND%20Studies%5BAll%20Fields%5D%29&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Ahlgren S., Orlova A., Wallberg H., Hansson M., Sandstrom M., Lewsley R., Wennborg A., Abrahmsen L., Tolmachev V., Feldwisch J. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
2 Sharkey R.M., Chang C.H., Rossi E.A., McBride W.J., Goldenberg D.M. (2012). Pretargeting: taking an alternate route for localizing radionuclides. Tumour Biol.
3 Tekabe Y., Einstein A.J., Johnson L.L., Khaw B.A. (2010). Targeting very small model lesions pretargeted with bispecific antibody with 99mTc-labeled high-specific radioactivity polymers. Nucl Med Commun.
4 Gada K.S., Patil V., Panwar R., Majewski S., Tekabe Y., Khaw B.A. (2011). Pretargeted gamma imaging of murine metastatic melanoma lung lesions with bispecific antibody and radiolabeled polymer drug conjugates. Nucl Med Commun.
5 Patil V., Gada K., Panwar R., Varvarigou A., Majewski S., Weisenberger A., Ferris C., Tekabe Y., Khaw B.A. (2012). Imaging small human prostate cancer xenografts after pretargeting with bispecific bombesin-antibody complexes and targeting with high specific radioactivity labeled polymer-drug conjugates. Eur J Nucl Med Mol Imaging.